# Folate-polyethylene glycol-ultrasmall superparamagnetic iron oxide nanoparticles

Chemical name: | Folate-polyethylene glycol-ultrasmall superparamagnetic iron oxide nanoparticles
Abbreviated name: | P1133
Synonym:
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules, which comprise ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or another polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material, which can range from ~10 to 3,500 nm in diameter, as large SPIO nanoparticles, standard SPIO nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (1).

Folic acid is a water-soluble B vitamin (2) that is essential for methylation and DNA synthesis. The primary pathway for folate entry into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity receptor (dissociation constant (K_d_) = 0.5 nM) that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells have been found to overexpress folate-binding protein (3). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the respective normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have also been found to express the folate receptor (4). Several folate-based conjugates have been studied in tumor imaging [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28%22folic%20acid%22%5BMeSH%20Terms%5D%20OR%20%28%22folic%22%5BAll%20Fields%5D%20AND%20%22acid%22%5BAll%20Fields%5D%29%20OR%20%22folic%20acid%22%5BAll%20Fields%5D%20OR%20%22folate%22%5BAll%20Fields%5D%29%20AND%20%28%22Receptor%22%5BJournal%5D%20OR%20%22receptor%22%5BAll%20Fields%5D%29%20AND%20%28%22molecular%20imaging%22%5BMeSH%20Terms%5D%20OR%20%28%22molecular%22%5BAll%20Fields%5D%20AND%20%22imaging%22%5BAll%20Fields%5D%29%20OR%20%22molecular%20imaging%22%5BAll%20Fiel)].

USPIO iron nanoparticles have diameters of 4–6 nm, and the hydrodynamic diameters with dextran or polyethylene glycol (PEG) coating are 20–50 nm. USPIO nanoparticles have a long plasma half-life because of their small size. The blood pool half-life is calculated to be ~24 h in humans (5) and 2 h in mice (6). Because of its long blood half-life, USPIO can be used as a blood pool agent during the early phase of intravenous administration (7). In the late phase, USPIO is suitable for the evaluation of the RES in the body, particularly in the lymph nodes (8). Various ligands and antibody-conjugated USPIO nanoparticles have been studied for in vivo targeted MRI in small animals (9, 10). Meier et al. (11) performed in vivo MRI of breast cancer in mice using folate-conjugated PEG-USPIO nanoparticles (P1133).

### Related Resource Links:

- Chapters in MICAD (Folate (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (Folate receptor (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor), USPIO (http://www.clinicaltrials.gov/ct2/results?term=uspio))
- Drug information in FDA (Folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133%20and%20synthesis)]

Meier et al. (11) prepared folate-PEG-amine by reaction of folic acid with PEG-bis-amine in anhydrous dimethyl sulfoxide with diisopropylcarbodiimide/N-hydroxysuccinimide. Folate-PEG-amine was purified with column chromatography. Folate-PEG-amine was added to carboxylate-USPIO nanoparticles. The product, P1133, had a mean hydrodynamic diameter of 26 nm. There were 8–10 folate moieties per nanoparticle. P904 (PEG-USPIO without folate; diameter, 21 nm) was also prepared as a control. P1133 exhibited an r1 relaxivity value of 12 mM^-1^s^-1^ and an r2 relaxivity value of 95 mM^-1^s^-1^ in water at 60 MHz. P904 showed r1 and r2 relaxivity values similar to those of P1133.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133%20and%20in%20vitro)]

Cells from human breast cancer cell line MDA-MB-231 express high levels of mRNA for folate receptor, whereas cells from the human lung carcinoma A549 have no detectable level (11). MDA-MB-231 cells (10 × 10^6^) were incubated with 50 µM P1133 and P904 with or without 750 µM folate for 24 h. P1133-Labeled MDA-MB-231 cells showed an iron uptake of 8.2 pg/cell, which was inhibited to 4.7 pg/cell with excess folate (P = 0.002). P904-Labeled cells (with or without excess folate) showed an iron uptake of 1.5 pg/cell. Untreated control cells showed iron levels of 0.68–0.73 pg/cell. The cell viability of P1133-labeled cells (95 ± 3%) was not significantly different from that of P904-labeled cells (97 ± 2%). MRI showed that P1133-labeled cells exhibited R2 relaxation rates of 0.0172 ms^-1^ and 0.0116 ms^-1^ without and with excess folate, respectively. Excess folate blocked uptake of P1133. P904-Labeled cells (with or without excess folate) showed R2 relaxation rates of ~0.0075–0.0079 ms^-1^, indicating that folate had little effect on the control P904. Untreated control cells showed R2 relaxation rates of 0.0071–0.0075 ms^-1^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133%20and%20rodentia)]

Meier et al. (11) performed a series of whole-body 3-T MRI (T2-weighted) in nude mice (n = 6) bearing MDA-MB-231 or A549 tumors after intravenous injection of 0.5 mmol Fe/kg P1133 and P904. Folate receptor–positive MDA-MB-231 tumors showed a moderate decline (P < 0.05) in signal/noise ratio (SNR) during the early phase (1 h) after injection of P1133 (21.1 ± 6.2) and P904 (19.7 ± 3.2) as compared with pre-injection (P1133 = 28.9 ± 6.0 and P904 = 27.4 ± 3.9). At 24 h, there was a persistent negative enhancement with P1133 (SNR = 14.9 ± 2.5, P = 0.011) but not with P904 (SNR = 27.0 ± 3.8, P = 0.29). The early-phase (1 h) negative enhancement was due to non-target perfusion retention in the tumors, and the later-phase (24 h) enhancement was due to P1133 targeting the folate receptor–positive tumors. On the other hand, folate receptor–negative A549 tumors showed a minor negative enhancement during the early phase and did not show a persistent negative enhancement during the later phase. Immunohistochemical staining confirmed the presence of folate receptors in MDA-MB-231 tumors and the absence of folate receptors in A549 tumors. P1133-Treated MDA-MB-231 tumors exhibited intracellular and extracellular retention of iron particles, but the same was not observed in P1133-treated A549 tumors, P904-treated MDA-MD-231 tumors, or P904-treated A549 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=P1133%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
3 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
4 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
5 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
6 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
7 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
8 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
9 Boutry S., Laurent S., Elst L.V., Muller R.N. (2006). Specific E-selectin targeting with a superparamagnetic MRI contrast agent. Contrast Media Mol Imaging.
10 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
11 Meier R., Henning T.D., Boddington S., Tavri S., Arora S., Piontek G., Rudelius M., Corot C., Daldrup-Link H.E. (2010). Breast cancers: MR imaging of folate-receptor expression with the folate-specific nanoparticle P1133. Radiology.